# [^123^I]-2-Iodo-2-amino-3-phenylpropanoic acid

Chemical name: | [^123^I]-2-Iodo-2-amino-3-phenylpropanoic acid
Abbreviated name: | 2-[^123^I] I-L-PA
Synonym: | 2-[^123^I]-iodo-L-phenylalanine
Agent Category: | Compound
Target: | Tumors
Target Category: | Transport through L-type amino acid transporter
Method of detection: | Single-photon emission computed tomography (SPECT); planar gamma imaging
Source of Signal/Contrast: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure of 2-[^123^I]-iodo-L-phenylalanine for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+iodo+L+phenylalanine)]

Although [^18^F]fluoro-deoxyglucose ([^18^F]FDG) is often used for the detection of malignant tumors, it has limitations because the radiochemical is also nonselectively taken up by inflamed or infected tissue (1-3). Compared with [^18^F]FDG, labeled amino acids (aa) such as ¹¹C-methionine, ^18^F-tyrosine, and their derivatives have been shown to be superior at distinguishing tumors from infection or inflammation in humans because these radiochemicals are taken up by the cells through a specialized transport system that has an upregulated expression in proliferating cells (4). The upregulation was observed primarily in cells of the tumor tissue, and normal tissue shows little change in expression of the aa transporters (because the cells divide slowly and only when necessary). This phenomenon is believed to be necessary for tumor cell survival because it supports the increased aa demand for protein synthesis in the rapidly dividing cells (5). One of the transporters, described as the major vehicle of large, neutral aa such as phenylalanine, leucine, and tyrosine, is known as the L system (L-type aa transporter 1; LAT1) and is independent of sodium for the transport of these aa (5). Different compounds, including aa, labeled with radioactive fluorine (^18^F) or carbon (^11^C) have been used to study tumors and to predict survival after radiotherapy with positron emission tomography (PET) (6-8). However, PET is not widely available, and investigators have developed aa probes that can be used with single-photon emission computed tomography (SPECT) to study tumors because this method is more available than PET (9).

Labeled with radioactive iodine (as ^123^I or ^125^I), aa derivatives such as 2-iodo-L-tyrosine, 4-iodo-L-phenylalanine, and 2-iodo-L-phenylalanine (2I-L-PA) were developed and observed to accumulate in rhabdomyosarcoma (R1M) tumor cells without incorporation into proteins. These derivatives could be used with SPECT to detect malignant tissue (10-12). Several studies, including in vitro studies, that used 2-[^123^I]I-L-PA to investigate the detection of tumors and biodistribution in rats, mice, dogs, and humans are available (13-17).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+2+iodo+L+phenylalanine+synthesis)]

The synthesis and labeling of 2I-L-PA with ^123^I was described by Kersemans et al. (12). A Cu^1+^ non-isotopic exchange method was used to synthesize 2I-L-PA as described elsewhere (18). Briefly, 2-bromo-L-phenylalanine was mixed with copper sulphate (CuSO_4_), tin sulphate (SnSO_4_), gentisic acid, and sodium iodide. The solution was flushed with nitrogen gas for 10 min and heated at 160°C for 16 h in a nitrogen atmosphere. The solution was centrifuged, and the products were transferred to a new flask to evaporate all the water. The contents were then purified with high-performance liquid chromatography (HPLC) on a Hibar Lichrosorb RP-select column, and further purification of the product was achieved by repeated dissolving in methanol coupled with evaporation of the solvent. Identification and quality control of the product was performed with nuclear magnetic resonance imaging, liquid chromatography mass spectroscopy, thin-layer chromatography, and HPLC. Chiral chromatography showed that there was no chiral modification to 2-iodo-D-phenylalanine. The yield of this reaction was reported to be 65% (12).

Radioiodination with ^123^I or ^125^I was performed as described by Kersemans et al. under acidic and reducing conditions (12). ^123^I or ^125^I was mixed with 2I-L-PA in the presence of CuSO_4_, SnSO_4_, gentisic acid, and citric acid; the solution was heated at 100°C for 60 min. The reaction was terminated with trisodium citrate dehydrate to obtain an isotonic solution with a pH of at least 4.0. The reaction mixture was then filtered through a silver filter (0.22 μm thick) to sterilize the product and to remove all the free ^123/125^I. HPLC on a Sep-Pak C18 column was used to identify the product and control the quality. Chiral chromatography was performed to confirm the absence of any 2-iodo-D-phenylalanine. The radiochemical yield of the iodinations was not reported; the radiochemical purity was >99% with specific activity of 65 GBq/mmol (1.75 Ci/mmol) for the ^123^I and 11 GBq/mmol (0.297 Ci/mmol) for the ^125^I labeling. The in vivo stability of the halogenated compound ([^125^I]2I-L-PA) was reported to be 92.7% (7.3% of the radiochemical was dehaloginated) as determined by HPLC. No other degradation products were detected. Ethylendiamine tetraacetic acid did not change dehalogination of the radiotracers (12).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+2+iodo+L+phenylalanine+in+vitro)]

The in vitro uptake of [^125^I]2I-L-PA was studied in R1M rat rabdomyosarcoma cells in the presence or absence of Na^+^ ions in MEM buffer (14). The uptake of [^125^I]2I-L-PA was observed to be a reversible, pseudo–first-order reaction in presence or absence of Na^+^ ions, and the radiochemical was not incorporated into the cell proteins. Uptake was shown to occur with the same affinity as L-phenylalanine through a saturable transport system that was inhibited competitively by 2-amino-2-norbornane-carboxylic acid, which selectively uses the L transport system. The transport system used by [^125^I]2I-L-PA was shown to be of the LAT1 type (14).

The in vitro uptake of [^125^I]2I-L-PA was also studied in R1M cells irradiated with cobalt (^60^Co) gamma rays and non-irradiated (control) R1M cells (9). Uptake was reported to be higher in cells that survived the radiation treatment than in cells that were not irradiated.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+2+iodo+L+phenylalanine+rodentia)]

The uptake of 2-[^123/125^I]I-L-PA was studied with dynamic planar imaging (DPI) in athymic mice bearing R1M cell tumors and NMRI mice with acute inflammation (12). The displacement of 2-[^123^I]I-L-PA by L-phenylalanine, L-methionine, and L-cysteine in these animals was also investigated. Magnetic resonance imaging was used to visualize the tumors in DPI. For comparison, the uptake of [^18^F]FDG was compared with the uptake of 2-[^125^I]I-L-PA in inflamed muscles of the mice. A high, fast, and reversible tumor uptake of 2-[^123/125^I]I-L-PA was reported with a tumorbackground ratio of 6.7 at 60 min. The radiolabeled aa was displaced by L-phenylalanine, L-methionine, or L-cysteine, which indicates that the aa used a reversible LAT transport system. The label was cleared rapidly through the kidneys, and a low accumulation of the tracer was observed in the abdomen and the brain. Compared with [^18^F]FDG, only a small amount of 2-[^125^I]I-L-PA was observed in inflamed tissue (inflammation/background ratio of 11.1 ± 1.7 Vs 1.3 ± 0.02, respectively) (12).

With the use of DPI and dissection, Kersemans et al. compared the biodistribution of 2-[^123^I]I-L-PA with that of 2-[^123^I]-iodo-L-tyrosine in athymic mice bearing rhabdomyosarcoma tumors (13). Competition studies with L-phenylalanine were also performed to confirm specificity of the tumor uptake. The biodistribution of 2-[^123^I]I-L-PA and 2-[^123^I]-iodo-L-tyrosine was also compared with that of [^18^F]FDG in these animals. No significant difference was observed between the tumor uptake values of 2-[^123^I]I-L-PA or 2-[^123^I]-iodo-L-tyrosine, and both tracers were reported to show a rapid, high, and specific accumulation in the tumors. Among the two radiochemicals, 2-[^123^I] I-L-PA showed a faster clearance from blood through the kidneys. Compared with the slight accumulation of 2-[^123^I] -iodo-L-tyrosine in the liver, there was no retention of 2-[^123^I] I-L-PA in this organ. Both 2-[^123^I]I-L-PA and 2-[^123^I]-iodo-L-tyrosine appeared to be superior to [^18^F]FDG for the detection of tumors in the brain and heart because these radiochemicals showed lower accumulation in these organs (see Table 4 in Kersemans et al. (13) for comparison).

In another study, the methods of sedation and data acquisition for 2-[^123^I]I-L-PA were shown to influence the uptake and biodistribution of this tracer in the various organs in athymic mice bearing R1M tumors (19). Mice treated with phenobarbital and untreated mice were injected with 2-[^123^I]I-L-PA, and an analysis of variance, t test, and clustered boxplot analysis were used to compare the results between the treated and untreated animals. Pentobarbital was reported to reduce the blood clearance and distribution of 2-[^123^I]I-L-PA toward the peripheral tissue of the animals. These factors were shown to influence the tumor/background ratios as well as nuclear imaging when the animals were treated with phenobarbital. The investigators recommended that the quantitative influence of sedation and the data acquisition methods should be investigated and taken into consideration for interpretation of the results in animal experiments with 2-[^123^I]I-L-PA (19).

Bauwens et al. used dynamic and static gamma planar imaging to compare the biodistribution, tumor uptake, and retention of D- and L-2-[^123^I]I-PA to D- and L-2-[^123^I]I-tyrosine in Wag/Rij rats bearing R1M tumors (17). The differential uptake ratios of D- and L-2-[^123^I]I-PA to D- and L-2 -[^123^I]I-tyrosine were reported to be 2.1, 2.3, 2.5, and 1.7, respectively, and they reached a maximum between 10 and 30 min after the injection. Both D- and L-2-[^123^I] I-PA showed an almost equal retention in the tumors for up to 48 h that was higher than either D- and L-2-[^123^I] I-tyrosine (17).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+2+iodo+L+phenylalanine+dogs)]

Using gamma planar imaging, Peremans et al. investigated the uptake of 2-[^123^I]I-L-PA in two dogs with synovial cell carcinoma of the tarsus (15). The tracer was observed to accumulate in the tumors (0.8% of the total injected activity) with a tumor/background contrast of 1.85 ± 0.52 at 10 min after administration in one dog; the ratio was 1.84 in the second animal. No metastases were detected with this tracer, which was cleared primarily through the kidneys in these animals.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+2+iodo+L+phenylalanine+non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+2+iodo+L+phenylalanine+humans)]

Bauwens et al. investigated the biodistribution and dosimetry of D and L isomers of 2-[^123^I]I-PA in five healthy human volunteers (16). For intra-individual comparison, the subjects received both the D and L isomers of 2-[^123^II-PA with a 1-week interval between the treatments. Blood and urine samples were collected after the treatment, and whole-body imaging was performed for up to 24 h after administration of the tracers. Both radiochemicals showed a moderate uptake in the heart and liver; with the most accumulation found in the muscle tissue. Clearance for both isomers was through the urinary system, and the bladder wall received/absorbed the highest dose. The effective radiation doses for the D and L isomers were determined to be 0.0106 ± 0.0038 mSv × Bq^-1^ and 0.0120 ± 0.0020 mSv × Bq^-1^, respectively. Between the two enantomers, 2-[^123^I]I-D-PA was reported to have a faster clearance, which resulted in a lower dose and reduced background in the subjects.

## Supplemental Information

[Disclaimers]

## References

1 Bleeker-Rovers C.P., Vos F.J., Corstens F.H., Oyen W.J. (2008). Imaging of infectious diseases using [18F] fluorodeoxyglucose PET. Q J Nucl Med Mol Imaging.
2 Rudd J.H., Myers K.S., Bansilal S., Machac J., Pinto C.A., Tong C., Rafique A., Hargeaves R., Farkouh M., Fuster V., Fayad Z.A. (2008). Atherosclerosis Inflammation Imaging with 18F-FDG PET: Carotid, Iliac, and Femoral Uptake Reproducibility, Quantification Methods, and Recommendations. J Nucl Med.
3 Ueda S., Tsuda H., Asakawa H., Shigekawa T., Fukatsu K., Kondo N., Yamamoto M., Hama Y., Tamura K., Ishida J., Abe Y., Mochizuki H. (2008). Clinicopathological and prognostic relevance of uptake level using 18F-fluorodeoxyglucose positron emission tomography/computed tomography fusion imaging (18F-FDG PET/CT) in primary breast cancer. Jpn J Clin Oncol.
4 Groves A.M., Win T., Haim S.B., Ell P.J. (2007). Non-[18F]FDG PET in clinical oncology. Lancet Oncol.
5 Yanagida O., Kanai Y., Chairoungdua A., Kim D.K., Segawa H., Nii T., Cha S.H., Matsuo H., Fukushima J., Fukasawa Y., Tani Y., Taketani Y., Uchino H., Kim J.Y., Inatomi J., Okayasu I., Miyamoto K., Takeda E., Goya T., Endou H. (2001). Human L-type amino acid transporter 1 (LAT1): characterization of function and expression in tumor cell lines. Biochim Biophys Acta.
6 de Boer J.R., Pruim J., Albers F.W., Burlage F., Vaalburg W., van der Laan B.F. (2004). Prediction of survival and therapy outcome with 11C-tyrosine PET in patients with laryngeal carcinoma. J Nucl Med.
7 Ishimori T., Saga T., Nagata Y., Nakamoto Y., Higashi T., Mamede M., Mukai T., Negoro Y., Aoki T., Hiraoka M., Konishi J. (2004). 18F-FDG and 11C-methionine PET for evaluation of treatment response of lung cancer after stereotactic radiotherapy. Ann Nucl Med.
8 Sugiyama M., Sakahara H., Sato K., Harada N., Fukumoto D., Kakiuchi T., Hirano T., Kohno E., Tsukada H. (2004). Evaluation of 3'-deoxy-3'-18F-fluorothymidine for monitoring tumor response to radiotherapy and photodynamic therapy in mice. J Nucl Med.
9 Kersemans V., Vergote V., de Gelder V., Madani I., Thierens H., De Neve W., Mertens J., Slegers G., Burvenich C., Peremans K., De Spiegeleer B. (2008). The use of [123I]-2-iodo-L-phenylalanine as an early radiotherapy evaluation tool: in vitro R1M Rabdomyosarcoma cell and in vivo mouse experiments. Cancer Biother Radiopharm.
10 Samnick S., Schaefer A., Siebert S., Richter S., Vollmar B., Kirsch C.M. (2001). Preparation and investigation of tumor affinity, uptake kinetic and transport mechanism of iodine-123-labelled amino acid derivatives in human pancreatic carcinoma and glioblastoma cells. Nucl Med Biol.
11 Kersemans V., Cornelissen B., Bacher K., Kersemans K., Thierens H., Dierckx R.A., De Spiegeleer B., Slegers G., Mertens J. (2005). In vivo evaluation and dosimetry of 123I-2-iodo-D-phenylalanine, a new potential tumor-specific tracer for SPECT, in an R1M rhabdomyosarcoma athymic mouse model. J Nucl Med.
12 Kersemans V., Cornelissen B., Kersemans K., Bauwens M., Achten E., Dierckx R.A., Mertens J., Slegers G. (2005). In vivo characterization of 123/125I-2-iodo-L-phenylalanine in an R1M rhabdomyosarcoma athymic mouse model as a potential tumor tracer for SPECT. J Nucl Med.
13 Kersemans V., Cornelissen B., Kersemans K., Dierckx R.A., De Spiegeleer B., Mertens J., Slegers G. (2006). Comparative biodistribution study of the new tumor tracer [123I]-2-iodo-L-phenylalanine with [123I]-2-iodo-L-tyrosine. Nucl Med Biol.
14 Mertens J., Kersemans V., Bauwens M., Joos C., Lahoutte T., Bossuyt A., Slegers G. (2004). Synthesis, radiosynthesis, and in vitro characterization of [125I]-2- iodo-L-phenylalanine in a R1M rhabdomyosarcoma cell model as a new potential tumor tracer for SPECT. Nucl Med Biol.
15 Peremans K., Kersemans V., Liuti T., Vandermeulen E., Cornelissen B., Gielen I., De Spiegeleer B., Mertens J., Burvenich C., Slegers G. (2007). Use of [123I]-2-iodo-L-phenylalanine as a tumor imaging agent in two dogs with synovial cell sarcoma. Vet Radiol Ultrasound.
16 Bauwens M., Keyaerts M., Lahoutte T., Kersemans K., Caveliers V., Bossuyt A., Mertens J. (2007). Intra-individual comparison of the human biodistribution and dosimetry of the D and L isomers of 2-[123I]iodo-phenylalanine. Nucl Med Commun.
17 Bauwens M., Lahoutte T., Kersemans K., Caveliers V., Bossuyt A., Mertens J. (2007). D- and L-[123I]-2-I-phenylalanine show a long tumour retention compared with D- and L-[123I]-2-I-tyrosine in R1M rhabdomyosarcoma tumour-bearing Wag/Rij rats. Contrast Media Mol Imaging.
18 Yu J., Zolle I., Mertens J., Rakias F. (1995). Synthesis of 2-[131I]iodophenyl-metyrapone using Cu(I)-assisted nucleophilic exchange labelling: study of the reaction conditions. Nucl Med Biol.
19 Kersemans V., De Spiegeleer B., Mertens J., Slegers G. (2006). Influence of sedation and data acquisition method on tracer uptake in animal models: [123I]-2-iodo-L-phenylalanine in pentobarbital-sedated tumor-bearing athymic mice. Nucl Med Biol.